# Acetyl-lys-lys-lys-lys-lys-cys-gly-cys-gly-gly-pro-leu-tyr-lys-lys-ile-ile-lys-lys-leu-leu-glu-ser-heparin-[^99m^Tc]

Chemical name: | Acetyl-lys-lys-lys-lys-lys-cys-gly-cys-gly-gly-pro-leu-tyr-lys-lys-ile-ile-lys-lys-leu-leu-glu-ser-heparin-[^99m^Tc]
Abbreviated name: | P483H-^99m^Tc
Synonym:
Agent Category: | Peptide
Target: | Leukocytes (unknown binding site)
Target Category: | Binding
Method of detection: | Single-photon emission computed tomography (SPECT) or gamma planar imaging
Source of signal: | ^99m^Tc
Activation: | No
Studies: | - In vitro; - Non-primate non-rodent mammals; - Humans

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=P483H)]

Because of their ability to accumulate at sites of infection and inflammation, the leukocyte and monocyte components of the white blood cell (WBC) have often been labeled under ex vivo conditions with radioisotopes such as indium (^111^In), meta-stable technetium (^99m^Tc), or radioactive compounds such as ^99m^Tc-gluceptate, [^67^Ga]gallium citrate, and ^99m^Tc-labeled antibodies, etc (1). Radiolabeling of leukocytes or monocytes involves the isolation of these cells from the WBC pool, a process that is slow and expensive, involves the handling of blood, and can lead to contamination of the samples. In addition, the labeled cells have a slow clearance from circulation and may be imaged up to 24 h after administration to allow time for accumulation at the site of infection or inflammation. Also, these imaging agents usually have a low signal-to-noise ratio, especially during the early time points, and show a high intestinal uptake that interferes with diagnostic imaging of the abdominal area (2).

Radioactively labeled monoclonal antibodies have been used for the imaging of infections, but these radiopharmaceuticals have limited application because they also have a slow clearance from circulation and are not always sensitive enough to detect pulmonary or bone infections (3, 4). In addition, labeled antibodies have been shown to induce transient neutropenia and the formation of human anti-mouse antibodies (HAMA) (4, 5). The HAMA response can limit the repeat use of the antibodies because it neutralizes and alters the biodistribution of the agent (6). The use of peptides to detect sites of infection or inflammation is an attractive option because these compounds are cheap and easy to synthesize, can be modified to suit target requirements, and show rapid clearance from circulation (7, 8). Chemotactic peptides have been developed and evaluated for the imaging of infections and inflammation, but these compounds have limitations because the buffer components used to label the peptides may influence their biodistribution characteristics (8). Moyer et al. identified and developed a heparin-binding peptide, P483, for the imaging of infections (9). The sequence of this peptide was based on the platelet factor-4 heparin-binding region. The peptide comprises 23 amino acids, was modified to contain a lysine-rich region to allow rapid renal clearance, and could be labeled with ^99m^Tc. The peptide was complexed with heparin and labeled with ^99m^Tc to generate ^99m^Tc-P483H, a peptide that targets leukocytes (9). Conjugation of the peptide with heparin enhanced the binding of the labeled peptide to WBC. The labeled peptide was evaluated for the imaging of infections in a rabbit model and also in humans (9, 10).

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=P483H+synthesis)]

The synthesis of ^99m^Tc-P483H was described by Moyer et al. (9). The P483 peptide was synthesized with commercially available amino acids by use of solid-phase technology on a peptide synthesizer with N-α-Fmoc protection (11). The peptide was then purified by preparative reverse-phase high-performance liquid chromatography (RP-HPLC) and lyophilized as a trifluoroacetate (TFA) salt. Purity and composition of the peptide was confirmed by RP-HPLC and fast atom bombardment or electrospray mass spectrometry. Details of confirmation of the peptide composition with mass spectrometry were not provided by the investigators.

The peptide-heparin complex (P483H) was obtained by mixing 0.94 pmol of the peptide with 1 United States Pharmacopiea unit of heparin. Using peptide and heparin analysis, the optimal stochiometric ratio between the peptide and heparin for leukocyte labeling and in vivo localization at the infection site was determined to be 6.9 (9). Minimal accumulation of the labeled peptide at the site of infection was observed if the ratio was <3 or >60 (9).

For labeling with ^99m^Tc, the TFA salt of P483 was reconstituted in saline and mixed with ^99m^Tc-labeled glucoheptonate (9). The reaction was allowed to proceed at room temperature for 15 min. For quality control, the labeled peptide was assayed by silica gel instant thin-layer chromatography (ITLC) using two different solvent systems. With the first solvent system (i.e., saturated saline), ^99m^Tc-P483 had an R_f_ between 0.0 and 0.7; ^99m^Tc-pertechnetate and ^99m^Tc-glucoheptonate had an R_f_ between 0.7 and 1.0. With the second solvent system (pyridine:acetic acid:water), the ^99m^Tc-microcolloids had an R_f_ between 0.0 and 0.2, and the other labeled species had an R_f_ between 0.2 and 1.0. Criteria for acceptable labeling was defined as radiochemical purity (RCP) >90%. The reaction yield was not provided in the publication (9). Specific activity of the labeled peptide was determined to be 60–100 mCi/100 nmol (2,220–3,700 MBq/100 nmol).

Heparin was added to the radiolabeled peptide once it passed the quality-control test to generate ^99m^Tc-P483H. The heparin-conjugated peptide was then evaluated with thin-layer chromatography using solvent saturation pads with acetonitrile:acetic acid:water as the solvent system. With this solvent system the heparin conjugate had an R_f_ between 0.0 and 0.5 (9).

Formulated kit vials were also prepared by adding 0.015–0.025 μM P483 as a TFA salt with or without heparin (9). These formulations also contained sufficient glucoheptonate, tin chloride, and buffers to produce an RCP >95% after the addition of ^99m^Tc-pertechnetate. The P483 kits without heparin were either reconstituted with ^99m^Tc-pertechnetate and then heparin was added to the labeled peptide, or vice versa (9). The ^99m^Tc-labeled peptides generated with the formulated kits were evaluated for quality, as detailed above, before use.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=P483H+in+vitro)]

To determine the in vitro association of ^99m^Tc-P483H, human whole blood was diluted and exposed to the labeled peptide-heparin conjugate (9). The labeled blood samples were then fractionated by density gradient centrifugation over Ficoll-Hypaque in neutrophil isolation medium. As a control, the blood samples were labeled with ^111^In and ^99m^Tc-gluceptate alone. On average 76.2% of the applied radioactivity was determined to be associated with the WBC; of the cell-associated activity, the polymorphonuclear cells had only 36%, whereas the leukocytes/monocytes had the remaining 64% of the label. Among these cells, 54% of the total label was associated with the monocytes. The investigators reported that labeling of the whole blood at room temperature for >8 h produced the same radioactivity distribution, indicating that the radiolabeled peptide was stable in whole blood for prolonged periods (9).

The in vitro labeling of purified WBC with ^111^In-oxine, ^99m^Tc-gluceptate, and ^99m^Tc-P483H was also compared by the investigators (9). Among these, ~73% of ^111^In and ^99m^Tc-P483H were associated with the WBC, but <15% ^99m^Tc-gluceptate was found with these cells. These results indicated that ^99m^Tc-P483H associated quantitatively with the WBC. Further isolation of monocytes from the lymphocytes indicated that ^99m^Tc-P483H was associated primarily with the monocytes (9). Such a distribution of radioactivity was not investigated for the ^111^In-labeled WBC.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=P483H+rhodentia)]

No references are currently available.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=P483H+Nonhuman+primates)]

The biodistribution of ^99m^Tc-P483H was investigated in rabbits and compared to the distribution of ^67^Ga-citrate, ^99m^Tc-gluceptate, ^131^I-albumin, ^99m^Tc-nanocolloid, ^111^In-WBC, and ^111^In-diethylenetriamene pentaacetic acid (9). New Zealand White rabbits were injected with the respective labeled compounds 18 to 24 h after infection with Escherichia coli in the left calf muscle. Imaging of the animals was performed 4 h after administration of the labeled compounds. ^99m^Tc-P483H was evaluated in 48 animals with the use of the various formulations. For the other radiochemicals the number of animals used varied from 1 to 5 (9). On average, 0.062 ± 0.029% of the injected dose (ID)/g of ^99m^Tc-P483H was detected in the infected tissue, and the infected/control tissue ratio was 26.8 ± 16.8, which was the highest among all the labeled compounds (9). A study of the time course of accumulation of label at the site of infection showed that ~1.8 to 2.0% ID/g was detected at the site 10–12 h after administration of the label. Detailed distribution of the compounds is provided in Table 2 of the publication by Moyer et al. (9). Similarly the infected tissue/blood ratio for ^99m^Tc-P483H was 3.1, which was higher than any other radiolabeled compound in the study.

In another study, the WBC were labeled with ^99m^Tc-P483H, washed of excess radioactivity, and administered to rabbits (n = 2) with E. coli–infected calf muscles (9). For comparison, another group of E. coli–infected rabbits were injected with ^111^In-WBC. The two compounds behaved similarly; during the early period both labels were detected in the lungs, but by 4 h after injection the contrast was evident at the infected site. On average, 0.0381 ± 0.022% ID/g tissue of ^99m^Tc-P483H–labeled WBC were detected at the infection site. No blocking studies were carried out.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28primate%20NOT%20human%29)]

No references are currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=P483H+humans)]

The safety and efficacy of ^99m^Tc-P483H for the detection of infection in humans was evaluated by Palestro et al. (10). In this study, the effects of peptide dose on performance were also determined, and results obtained with the peptide were compared to those obtained with in vitro–labeled leukocytes. Thirty patients were given three different doses of the labeled peptide (2.9 nmol (n = 11), 14.5 nmol (n = 10), 29.0 nmol (n = 9)) and imaged at 15 min and 90–120 min after the injection. Scintigraphy was also performed on 20 patients after the administration of autologous ^111^In-labeled leukocyte. Among these patients, 7 had osteomyelitis, 5 had vascular grafts, 2 had abscess, 1 had joint replacement, 1 had a surgical wound, and 1 had pneumonia. The sensitivity, specificity, and accuracy were determined to be 0.86, 0.81, and 0.83, respectively, for both imaging time points. From this study no correlation between the peptide dose and accuracy was apparent. Patients who underwent both procedures, labeled peptide and autologous in vitro–labeled leukocyte administration, followed by imaging had an identical accuracy of 80%. From this study the investigators concluded that ^99m^Tc-P483H was safe and able to detect infections rapidly and accurately. Imaging results obtained with the labeled peptide were comparable to those obtained with in vitro–labeled leukocytes.

## References

1 Boerman O.C., Rennen H., Oyen W.J., Corstens F.H. (2001). Radiopharmaceuticals to image infection and inflammation. Semin Nucl Med.
2 Ballinger J.R., Gnanasegaran G. (2005). Radiolabelled leukocytes for imaging inflammation: how radiochemistry affects clinical use. Q J Nucl Med Mol Imaging.
3 Rubin R.H., Fischman A.J. (1994). The use of radiolabeled nonspecific immunoglobulin in the detection of focal inflammation. Semin Nucl Med.
4 Becker W., Bair J., Behr T., Repp R., Streckenbach H., Beck H., Gramatzki M., Winship M.J., Goldenberg D.M., Wolf F. (1994). Detection of soft-tissue infections and osteomyelitis using a technetium-99m-labeled anti-granulocyte monoclonal antibody fragment. J Nucl Med.
5 Thakur M.L., Li J., Chandy B., John E.K., Gibbons G. (1996). Transient neutropenia: neutrophil distribution and replacement. J Nucl Med.
6 Sakahara H., Reynolds J.C., Carrasquillo J.A., Lora M.E., Maloney P.J., Lotze M.T., Larson S.M., Neumann R.D. (1989). In vitro complex formation and biodistribution of mouse antitumor monoclonal antibody in cancer patients. J Nucl Med.
7 Fischman A.J., Babich J.W., Rubin R.H. (1994). Infection imaging with technetium-99m-labeled chemotactic peptide analogs. Semin Nucl Med.
8 Lister-James J., Moyer B.R., Dean T. (1996). Small peptides radiolabeled with 99mTc. Q J Nucl Med.
9 Moyer B.R., Vallabhajosula S., Lister-James J., Bush L.R., Cyr J.E., Snow D.A., Bastidas D., Lipszyc H., Dean R.T. (1996). Technetium-99m-white blood cell-specific imaging agent developed from platelet factor 4 to detect infection. J Nucl Med.
10 Palestro C.J., Weiland F.L., Seabold J.E., Valdivia S., Tomas M.B., Moyer B.R., Baran Y.M., Lister-James J., Dean R.T. (2001). Localizing infection with a technetium-99m-labeled peptide: initial results. Nucl Med Commun.
11 Merrifield R.B. (1963). Solid-phase synthesis of peptides. Journal of American Chemical Society.